# N-{2-[4-(4-[^125^I]Iodobenzyl)-piperidin-1-ylmethyl]benzoimidazol-5-yl}-methanesulfonamide

Chemical name: | N-{2-[4-(4-[^125^I]Iodobenzyl)-piperidin-1-ylmethyl]benzoimidazol-5-yl}-methanesulfonamide
Abbreviated name: | [^125^I]9
Synonym:
Agent Category: | Compound
Target: | N-methyl-D-aspartate (NMDA) receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information on [^125^I]8 in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Functions%20of%20NMDA%20receptor&cmd=DetailsSearch)]

The N-methyl-D-aspartate (NMDA) receptor (NMDAR) belongs to a sub-group of the glutamate receptor family and has a heteromeric structure that is made up of three subunits (NR1, NR2, and NR3) as dimeric combinations (NR1/NR2 or NR1/NR3). There are four subtypes of NR2 (NR2A–NR2D), and NR3 has two subtypes, NR3A and NR3B. The NMDAR can bind several different types of ligands and has important functions in the process of learning and in the performance of memory tasks in a variety of animal species (invertebrate and vertebrate) (1, 2). These receptors are involved in the development of neurological conditions such as Parkinson’s disease, Alzheimer’s disease, bipolar disorder, etc (2, 3). The structure, distribution, and function of the NMDAR in the rodent brain has been reviewed elsewhere (1, 4). The NR1 subunit of the NMDAR is known to be distributed in all parts of the brain; of the different NR2 subtypes, NR2A is found throughout the brain, whereas NR2B, NR2C, and NR2D are present mainly in the forebrain (including the cerebral cortex, hippocampus, and the olfactory lobes), cerebellum, and the lower brain stem, respectively. High levels of the NR3A subtype are detected in many brain regions of only prenatal and newborn mice, whereas NR3B levels are low during these developmental stages. However, the NR3 subtype is expressed predominantly in the adult brain (4).

Among the different NR2 and NR3 subunits, primarily the NR2B subunit is believed to modulate the various physiological and pharmacological activities of the NMDAR as mentioned above. Attempts to study the distribution of the NMDAR that contains the NR2B subunit in the brain through the use of positron emission tomography with radiolabeled compounds have been unsuccessful because the tracers lack binding specificity for the receptor (3). However, among these tracers, inspite of a high non-specific uptake of 6-{3-[4-(4-fluorobenzyl)piperidino]propionyl}-3H-benzoxazol-2-[^11^C]-one ([^11^C]EMD-95885; a benzimidazole derivative) in the rodent brain the amount of radioactivity in the organ was reduced by pretreatment of the animals with ifenprodil, a selective antagonist of the NR2B subunit, suggesting that [^11^C]EMD-95885 could be a suitable platform for the development of new imaging probes to study the location and distribution of the NMDAR that contains the NR2B subunit in the rodent brain (3). Results from in vitro assays demonstrated that novel compounds with a structure resembling EMD-95885 maintained their affinity for the NR2B subunit (5). On the basis of this information, Fuchigami et al. synthesized a series of [^125^I]-labeled benzimidazole derivatives and investigated their in vitro receptor binding and in vivo brain uptake characteristics in normal mice (3). Among these radioiodinated compounds, only two, 2-{[4-(4-[^125^I]iodobenzyl)piperidin-1-yl]methyl}benzimidazol-5-ol ([^125^I]8) and N-{2-[4-(4-[^125^I]iodobenzyl)-piperidin-1-ylmethyl]benzoimidazol-5-yl}-methanesulfonamide ([^125^I]9), were shown to have a high affinity for the NR2B subunit under in vitro conditions. This chapter discusses the in vitro and in vivo results obtained with [^125^I]9; the characteristics of [^125^I]8 are described in a separate chapter of MICAD (www.micad.nih.gov) (6).

### Other Sources of Information

Other chapters on NMDAR in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=NMDA%20receptor%20AND%20micad%5Bbook%5D)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001177656.1) of NMDA1 receptor (zeta 1) (Grin1), transcript variant 2

Information regarding NMDAR on FDA site (http://google2.fda.gov/search?q=NMDA+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=12)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=NMDA+receptor) on NMDAR

NR2A subunit (http://www.ncbi.nlm.nih.gov/omim/138253) in OMIM (Online Mendelian Inheritance in Man database)

NR2B subunit (http://www.ncbi.nlm.nih.gov/omim/138252) in OMIM (Online Mendelian Inheritance in Man database)

## Synthesis

[PubMed]

The synthesis of [^125^I]9 and [^125^I]8 has been detailed by Fuchigami et al. (3). The radiochemical yields of [^125^I]9 and [^125^I]8 were reported to be 78%–81% and 85%–90%, respectively, based on the amount of [^125^I]sodium iodide used in the synthesis. The radiochemical purity values of the final product for both labeled compounds were >98% as determined with high-performance liquid chromatography. The specific activity and in vitro stability of [^125^I]9 and [^125^I]8 were not reported.

Using the shake-flask method, the partition coefficients of 9 and 8 between octanol and phosphate-buffered saline (pH 7.4) were determined to be 3.54 and 3.95, respectively (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=N-%7B2-%5B4-%284-%5B125I%5Diodobenzyl%29-piperidin-1-ylmethyl%5Dbenzoimidazol-5-yl%7D-methanesulfonamide%20in%20vitro&cmd=DetailsSearch)]

Using an in vitro [^3^H]ifenprodil displacement assay with rat cortical membrane homogenates, the K_i_ values of 9 and 8 were determined to be 5.75 ± 1.19 nM and 7.28 ± 2.93 nM, respectively (3).

In another study, the distribution of [^125^I]9 and [^125^I]8 on rat brain sections was investigated with an autoradiographic technique as described elsewhere (3). Radioiodinated 9 and 8 accumulated primarily in the forebrain (cerebral cortex and hippocampus; these regions are rich in NR2B), and a low level of the tracer was detected in the cerebellum, which exhibits low expression of NR2B. However, in general, both tracers showed a high non-specific binding in the brain sections. Pretreatment of the brain sections with Ro-25,6981, a NR2B-selective anatagonist, was shown to inhibit the binding of [^125^I]9 and [^125^I]8 in the different parts of the forebrain, indicating that the tracers probably had some specificity for the NR2B subunit of the NMDAR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=N-%7B2-%5B4-%284-%5B125I%5Diodobenzyl%29-piperidin-1-ylmethyl%5Dbenzoimidazol-5-yl%7D-methanesulfonamide%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]9 and [^125^I]8 was investigated in normal ddY mice (n = 5–6 animals/time point per tracer) as described by Fuchigami et al. (3). The animals were injected with the respective tracers through the tail vein and euthanized at predetermined time points to measure the amount of radioactivity that accumulated in the major organs. Data were presented as percent injected dose per gram tissue (% ID/g). Maximum uptake of [^125^I]9 and [^125^I]8 was observed in the liver, with an accumulation of 19.35 ± 9.22% ID/g and 25.03 ± 4.20% ID/g of the two compounds, respectively, at 5 min postinjection (p.i.), which increased to 17.81 ± 4.07% ID/g and 32.22 ± 6.56% ID/g, respectively, at 180 min p.i. Although the accumulation remained relatively constant for [^125^I]8 at 360 min p.i., accumulation decreased to 10.93 ± 2.51% ID/g for [^125^I]9 at this time point. In the kidneys, the accumulation was 10.99 ± 4.46% ID/g and 12.20 ± 3.18% ID/g for [^125^I]9 and [^125^I]8, respectively, at 5 min p.i. and increased to 10.51 ± 1.97% ID/g for [^125^I]9 at 360 min p.i., but decreased to 5.46 ± 0.67% ID/g for [^125^I]8 at this time point. The lungs showed an uptake of 9.07 ± 5.18% ID/g and 14.48 ± 2.52% ID/g for [^125^I]9 and [^125^I]8, respectively, at 5 min p.i. and decreased to 3.62 ± 0.21% ID/g and 3.44 ± 0.80% ID/g, respectively, at 360 p.i. In the brain, the accumulation was 0.32 ± 0.12 and 0.42 ± 0.06% ID/g for [^125^I]9 and [^125^I]8, respectively, at 5 min p.i., which increased to 0.47 ± 0.09% ID/g and 0.55 ± 0.14% ID/g, respectively, at 360 min p.i. The brain/blood (B/B) ratios for [^125^I]9 and [^125^I]8 increased from 0.46 ± 0.09 and 0.36 ± 0.03, respectively, at 5 min p.i. to 1.34 ± 0.28 and 2.23 ± 0.99, respectively, at 360 min p.i.

Because the brain uptake profile of [^125^I]8 appeared to be superior to that of [^125^I]9, the binding specificity of [^125^I]9 in the different regions of the brain was not investigated with blocking studies. Blocking studies performed with [^125^I]8 are discussed elsewhere (6).

On the basis of observations that there is a low, uniform uptake of both [^125^I]9 and [^125^I]8, respectively, in almost all regions of the rodent forebrain and little evidence that the two tracers bound specifically to the NMDAR that contains the NR2B subunit the investigators concluded that these radioiodinated compounds were probably not suitable for single-photon emission computed tomography imaging of the cerebral NMDAR.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=N-%7B2-%5B4-%284-%5B125I%5Diodobenzyl%29-piperidin-1-ylmethyl%5Dbenzoimidazol-5-yl%7D-methanesulfonamide%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=N-%7B2-%5B4-%284-%5B125I%5Diodobenzyl%29-piperidin-1-ylmethyl%5Dbenzoimidazol-5-yl%7D-methanesulfonamide%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Magnusson K.R., Brim B.L., Das S.R. (2010). Selective Vulnerabilities of N-methyl-D-aspartate (NMDA) Receptors During Brain Aging. Front Aging Neurosci.
2 Teng H., Cai W., Zhou L., Zhang J., Liu Q., Wang Y., Dai W., Zhao M., Sun Z. (2010). Evolutionary mode and functional divergence of vertebrate NMDA receptor subunit 2 genes. PLoS One.
3 Fuchigami T., Yamaguchi H., Ogawa M., Biao L., Nakayama M., Haratake M., Magata Y. (2010). Synthesis and biological evaluation of radio-iodinated benzimidazoles as SPECT imaging agents for NR2B subtype of NMDA receptor. Bioorg Med Chem.
4 Low C.M., Wee K.S. (2010). New insights into the not-so-new NR3 subunits of N-methyl-D-aspartate receptor: localization, structure, and function. Mol Pharmacol.
5 Borza I., Kolok S., Gere A., Nagy J., Fodor L., Galgoczy K., Fetter J., Bertha F., Agai B., Horvath C., Farkas S., Domany G. (2006). Benzimidazole-2-carboxamides as novel NR2B selective NMDA receptor antagonists. Bioorg Med Chem Lett.
6 Chopra, A., 2-{[4-(4-[125I]iodobenzyl)piperidin-1-yl]methyl}benzimidazol-5-ol. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.